# Lipiodol-loaded poly(oxyethylene)-block-poly(oxypropylene)-block-poly(oxyethylene) triblock copolymers/polyethylene glycol-nanoparticles

Chemical name: | Lipiodol-loaded poly(oxyethylene)-block-poly(oxypropylene)-block-poly(oxyethylene) triblock copolymers/polyethylene glycol-nanoparticles
Abbreviated name: | LPNCs
Synonym: | Lipodol-Pluronic/PEG-NP, Lipodol-Poloxamer/PEG-NP, Lipodol-PEO-PPO-PEO/PEG-NP
Agent Category: | Nanoparticles
Target: | Non-targeted probe, the reticuloendothelial system (RES)
Target Category: | Non-specific filling of blood vessels and tissues, phagocytosis by the RES
Method of detection: | Computed tomography (CT) and planar X-ray
Source of signal: | Iodine (I)
Activation: | No
Studies: | - In vitro; - Rodents | Click on PubChem SID (3730533 (http://pubchem.ncbi.nlm.nih.gov/summary/summary.cgi?sid=3730533)) for more information.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(lipiodol)+AND+(nanoparticles)&WebEnv=0__rCI2XIFci2CWu8ykubtzkAcbcldgkW4wTKXd8FfCbQHms_UuCnG0XSfvs69O1Gb1QIhSMnse0ij%40256128CE704ECD70_0127SID&WebEnvRq=1)]

Lipiodol-loaded poly(oxyethylene)-block-poly(oxypropylene)-block-poly(oxyethylene) (PEO-PPO-PEO) triblock copolymers/polyethylene glycol (PEG)-nanoparticles (LPNCs) are X-ray contrast agent preparations developed for contrast enhancement in computed tomography (CT) imaging (1). Lipiodol (http://www.medsafe.govt.nz/profs/datasheet/l/Lipiodolultrafluidinj.htm) is an iodized poppy seed oil (ethyl esters of iodized fatty acids of poppy seed oil with 480 mg of iodine/ml) that can be used as an X-ray contrast agent for lymphography and hysterosalpingography. It is commercially available for investigation but has not been approved by the United States Food and Drug Administration for clinical use in humans.

X-ray imaging techniques (planar and CT) depend on tissue density differences that provide the image contrast produced by X-ray attenuation between the area of interest and surrounding tissues (2). Contrast enhancement (opacification) with the use of contrast agents increases the degree of contrast and improves the differentiation of pathological processes from normal tissues. Because iodine, an element with high atomic density, causes high attenuation of X-rays within the diagnostic energy spectrum, water-soluble and reasonably safe iodinated contrast agents in intravenous injectable forms have been developed for clinical applications (3, 4). Water-soluble, intravenous X-ray contrast agents are generally organic iodine compounds that contain one or more tri-iodinated benzene rings. When injected intravenously, they are largely distributed in the extracellular fluid space and excreted unchanged by the kidneys. Contrast enhancement of a region of interest depends on the route of administration, delivery of the agent to the area by blood flow, and the final iodine concentration in the region (5, 6).

Intravenous injection of water-soluble X-ray contrast agents can be performed in conjunction with dynamic CT to improve the detectability of tissue pathologies (4, 5, 7). However, there are many limitations associated with this approach because of their nonspecificity and rapid extravasation from the circulation. Nanoparticle contrast media have also been developed to improve the circulation time and target specificity of contrast agents (8, 9). One possible approach involves encapsulation of water-soluble or -insoluble X-ray contrast agents in various nanoparticle carriers (1, 8, 10, 11). Although these nanoparticle carriers are naturally taken up by the reticuloendothelial system, they can be modified with specific targeting moieties to increase the affinity of nanoparticles for target tissues, organs, and cells (1, 11-13). Among the nanoparticle carriers, PEO-PPO-PEO triblock copolymers are macromolecular surfactants composed of poly(oxyethylene)-block-poly(oxypropylene)-block-poly(oxyethylene) (Pluronic or Poloxamer series). Through hydrophobic interactions between the PPO blocks, these surfactants undergo self-assembly into spherical micelles in aqueous solution above a critical temperature (14). These nanoparticles can expand and shrink rapidly in response to temperature changes (15-17). Bae et al. (14) prepared LPNCs with the use of a new class of PEO-PPO-PEO/PEG nanoparticles to encapsulate lipiodol oil. LPNCs have an inner hydrophobic oil phase stabilized by a covalently cross-linked PEO-PPO-PEO/PEG shell layer. Kong et al. (1) reported that this LPNC nanoparticle preparation has effective X-ray attenuation properties and longer circulation time than those of conventional water-soluble contrast agents. The authors suggested that the conjugation of an appropriate targeting moiety might lead to the active targeting of LPNCs to a specific tissue or organ.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(lipiodol)+AND+(nanoparticles)&WebEnv=0OqooCb5TyGAuhIrtZxySoy-Q1guZmfbyftWQsivyIZlWsFay9u2eA--EwCXsGmg-IeCTPuNZoeVow%40256128CE704ECD70_0127SID&WebEnvRq=1)]

Bae et al. (14) reported the synthesis of LPNCs by the use of an emulsification/solvent evaporation method (15, 16). LPNCs were prepared by cross-linking the outer shell layers of PEO-PPO-PEO/PEG copolymer ((PEO)_100_(PP)_65_(PEO)_100_, Pluronic F127, Mw = 12,600) micelles reactively preactivated with amine. F127 was chosen because of its high hydrophilic/lipophilic balance value, high extractability in the aqueous phase, relatively low toxicity, and characteristic self-assembly into micelles. Briefly, F127 was first preactivated with p-nitrophenyl chloroformate (p-NPC) at its two terminal hydroxyl groups (1). Lipiodol was dissolved in dichloromethane and then mixed with the activated PEO-PPO-PEO/PEG copolymer. The mixture was added dropwise to a solution of amine-functionalized polyethylene glycol (pH 9) with six branches (PEG-amine_2_). This was sonicated for 3 min to form an oil-in-water emulsion, and it was then neutralized by hydrochloric acid. At this stage, the NPC group of the activated F127 was conjugated with the primary amine groups of the PEG-amine_2_ in the outer shells of the LPNCs. Residual dichloromethane was quickly removed from the resultant oil-in-water emulsion with a rotary evaporator. During this solvent removal process, the influx of water and the concomitant outflow of methylene chloride caused a phase separation into micelles. Methylene chloride exuded into the outer aqueous, phase-produced, oil-filled core at the interiors of the micelles. Cross-linking of the micelle outer shell layers by the PEG-amine_2_ prevented the fusion of the micelles with other micelles. The preparation was dialyzed using a dialysis membrane with a molecular mass cutoff of 50 kDa and then finally filtered by a 0.45 μm filter. The encapsulation efficiency of lipiodol was ~82% at a 100% F127/lipiodol weight ratio (w/w) (1). The authors suggested that there was no volume transition at the 100% (w/w) ratio of lipiodol/F127 (1, 14). The mean amount of encapsulated lipiodol was 71.1 ± 4.2% (w/w) of dried LPNCs.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(lipiodol)+AND+(nanoparticles)&WebEnv=04jqaAnCFKuJXlSNaqCLPSvwNMhl7vCvc9mw4OxCpnrEnZ69AQrJWe0tlpCQ3wheGsZlWxAY2MTnFD%40256128CE704ECD70_0127SID&WebEnvRq=1)]

The LPNC in vitro hydrodynamic diameter, dispersion stability, and volume transition in aqueous solution were evaluated with dynamic light scattering (1). The mean hydrodynamic diameters of LPNCs were 153.2 ± 14.4 nM (n = 3) and were stable for 72 h at 9–37ºC. The morphological characteristics of LPNCs were examined with scanning electron microscopy (SEM) and transmission electron microscopy (TEM). The SEM study showed that LPNCs maintained their spherical shape with a mean diameter of 150.4 ± 22.4 nm, and that LPNCs were well segregated and dispersed. The TEM study also showed well-dispersed LPNCs with high electron density and an average size of 146.3 ± 26.8 nm. At an LPNC concentration of 400 mg/ml, strong X-ray attenuation characteristics were demonstrated. There was no significant viscosity or aggregation at this concentration. In a release test of LPNCs in phosphate-buffered saline (pH 7.4) containing 0.02% (w/v) Tween 20 at 37ºC, no significant lipiodol outflow into the aqueous phase occurred during a period of 72 h (1).

The in vitro cytotoxicity of LPNCs was tested in A549 cells by the 2,3-bis(2-methoxy-4-nitro-5-sulfophenyl)-2H-tetrazolium-5-carboxanilide inner salt assay (1). The effective concentration of reducing the cell viability by 50% (EC_50_) was 0.196 mM iodine. In comparison, the EC_50_ for iopromide, a clinically used water-soluble CT contrast agent, was 0.0648 mM iodine.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(lipiodol)+AND+(nanoparticles)&WebEnv=0cny8Uan4RTE774tEXSqGXRie7VlWn5Ja-VWWma0P3OE7g_7GP3IQ4Jr9iU7iPeNu54DP9YP3kGLOL%40256128CE704ECD70_0127SID&WebEnvRq=1)]

Kong et al. (1) evaluated the X-ray contrast performance of LPNCs in mice by injecting 200 μl (400 mg/ml) LPNCs intravenously into healthy nude mice. CT imaging showed that the LPNCs contrast enhancement resulted in the clear delineation of the cardiac ventricles and major arterial and venous structures for 4 h after administration. Most LPNCs accumulated in the spleen and liver within 24 h. The contrast enhancement of the spleen and liver gradually faded during the time period of 24–72 h. Histological analysis at 72 h after administration showed decrement of lymphatic cells in the spleen, liver, and lymph nodes. Kong et al. (1) suggested that this supported the belief that there was nonspecific scavenging of LPNCs in the reticuloendothelial system.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((lipiodol)+AND+(nanoparticles))+AND+(dog+OR+rabbit+OR+pig+OR+sheep)&WebEnv=0bLB6OC2GXavB_MTV0i3XxQQrgFvIyzOLvP_q0LXFsnjdx98rbq0vQg-EZp3wh-qc7FCnSWvwU6_fG%40256128CE704ECD70_0127SID&)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((lipiodol)+AND+(nanoparticles))+AND+(primate+NOT+human))+AND+(primate+NOT+human)&WebEnv=0mBNqoQNIdTzeTaW5jfSlzZyVztwPoC1NC9Tvg-YUgID09v0OiKZivWJ7Cg3OmaWXzPXn1Zkl5vsP4%40256128CE704E)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((lipiodol)+AND+(nanoparticles))+AND+human&WebEnv=0rAFqaUnYTnNVolvm0HPLxQ3svBpsQfNn-aiby4Q325HDm8JMIYfO87P9MaJZd_Mu84PZBHJ5ox4PS%40256128CE704ECD70_0127SID&WebEnvRq=1)]

No publication is currently available.

## References

1 Kong W.H., Lee W.J., Cui Z.Y., Bae K.H., Park T.G., Kim J.H., Park K., Seo S.W. (2007). Nanoparticulate carrier containing water-insoluble iodinated oil as a multifunctional contrast agent for computed tomography imaging. Biomaterials.
2. Hoey, G.B. and K.R. Smith, Chemistry of X-ray contrast media, in Radiocontrast agents, M. Sovak, Editor. 1984, Springer-Verlag: New York. p. 23-125.
3 Wallingford V.H. (1953). The development of organic iodine compounds as x-ray contrast media. J Am Pharm Assoc Am Pharm Assoc (Baltim).
4. Swanson, D.P. and M.B. Alpern, Contrast media for computed tomography: Intravascular, intracavitary, xenon, reticuloendothelial, in Pharmaceuticals in medical imaging, D.P. Swanson, H. M. Chilton and J. H. Thrall, Editor. 1990, Macmillan Publishing Company: New York. p. 99-124.
5 Sovak M., Ranganathan R., Lang J.H., Lasser E.C. (1977). and Concepts in design of improved intravascular contrast agents. European Society of cardiovascular Radiology, Uppsala, (May): p. 25-27.
6 Almen T. (1969). Contrast agent design. Some aspects on the synthesis of water soluble contrast agents of low osmolality. J Theor Biol.
7. Hoey, G.B. and K.R. Smith, Chemistry of X-ray contras media, in Radiocontrast agents, M. Sovak, Editor. 1984, Springer-Verlag: New York. p. 23-125.
8 McIntire G.L., Bacon E.R., Toner J.L., Cornacoff J.B., Losco P.E., Illig K.J., Nikula K.J., Muggenburg B.A., Ketai L. (1998). Pulmonary delivery of nanoparticles of insoluble, iodinated CT X-ray contrast agents to lung draining lymph nodes in dogs. J Pharm Sci.
9 Rabin O., Manuel Perez J., Grimm J., Wojtkiewicz G., Weissleder R. (2006). An X-ray computed tomography imaging agent based on long-circulating bismuth sulphide nanoparticles. Nat Mater.
10 Cheng K.T., Seltzer S.E., Adams D.F., Blau M. (1987). The production and evaluation of contrast-carrying liposomes made with an automatic high-pressure system. Invest Radiol.
11 Yokoyama M. (2005). Drug targeting with nano-sized carrier systems. J Artif Organs.
12 Elmi M.M., Sarbolouki M.N. (2001). A simple method for preparation of immuno-magnetic liposomes. Int J Pharm.
13 Bianco A., Kostarelos K., Partidos C.D., Prato M. (2005). Biomedical applications of functionalised carbon nanotubes. Chem Commun (Camb).
14 Bae K.H., Lee Y., Park T.G. (2007). Oil-encapsulating PEO-PPO-PEO/PEG shell cross-linked nanocapsules for target-specific delivery of paclitaxel. Biomacromolecules.
15 Choi S.H., Lee S.H., Park T.G. (2006). Temperature-sensitive pluronic/poly(ethylenimine) nanocapsules for thermally triggered disruption of intracellular endosomal compartment. Biomacromolecules.
16 Choi S.H., Lee J.H., Choi S.M., Park T.G. (2006). Thermally reversible pluronic/heparin nanocapsules exhibiting 1000-fold volume transition. Langmuir.
17 Bae K.H., Choi S.H., Park S.Y., Lee Y., Park T.G. (2006). Thermosensitive pluronic micelles stabilized by shell cross-linking with gold nanoparticles. Langmuir.